# (R,S)-1,2,3,4,10,14b-Hexahydro-2-[^11^C]methylpyrazino(2,1-a)pyrido(2,3-c)(2)benzazepine

Chemical name: | (R,S)-1,2,3,4,10,14b-Hexahydro-2-[^11^C]methylpyrazino(2,1-a)pyrido(2,3-c) (2)benzazepine
Abbreviated name:
Synonym: | [^11^C]Mirtazapine
Agent category: | Compound
Target: | α_2_-Adrenoceptors
Target category: | Receptor
Method of detection: | Positron emission tomography (PET)
Source of signal: | ^11^C
Activation: | No
Studies: | - In vitro; - Other non-primate mammals; - Humans | Click on the above structure for additional information in PubChem (http://pubchem.ncbi.nlm.nih.gov/).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=11C%20Mirtazapine)]

Malfunction of the sympathetic nervous system may play a primary role in the pathogenesis of heart diseases. There are two subtypes of α-adrenoceptors, α_1_ and α_2_, in the heart. α-Adrenoceptors play a backup role for β_1_-adrenoceptors (1). The cardiac adrenoceptors are responsible for the regulation of heart rate and myocardial contractility (2). About 15% of cardiac adrenoceptors are α_1_-adrenoceptors. Presynaptic α_1_-adrenoceptors modulate noradrenalin release. α_1_-Adrenoceptors are present predominately in larger blood vessels, whereas α_2_-adrenoceptors are more prominent in smaller blood vessels. Increases in α_1_-adrenoceptor sites are usually observed when the number of β-adrenoceptors decreases in heart diseases (3). Imaging of the pathologic changes of adrenergic receptors offers a non-invasive assessment of myocardial diseases.

In the brain, high densities of α_2_-adrenoceptors are in the hippocampus, amygdala, basal ganglia, cortex, thalamus, hypothalamus, and hypothalamus (4). Changes in α_2_-adrenoceptor function have been implicated in Alzheimer’s disease, movement disorders, and depression (4, 5). (R,S)-1,2,3,4,10,14b-Hexahydro-2-methylpyrazino(2,1-a)pyrido(2,3-c) (2)benzazepine (mirtazapine) is active at central α_2_-adrenoceptors with proven clinical efficacy in the treatment of depression [PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=Mirtazapine%20and%20depression)]. It also is an antagonist to 5-HT_2_ and 5-HT_3_ receptors based on in vivo pharmacologic studies in animals (6). However, the antidepressant effects of mirtazapine are attributed primarily to inhibition of α_2_-adrenoceptors (7). Mirtazapine plays a role in the regulation of neurotransmitter release. To clarify any putative changes and to define the anatomical distribution of α_2_-adrenoceptors in vivo, [^11^C]mirtazapine is being developed as a positron emission tomography (PET) agent for the non-invasive study of antidepressant actions on α_2_-adrenoceptors in the brain.

### Related Resource Links:

- Chapters in MICAD (Adrenoceptors (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=books&Cmd=DetailsSearch&Term=adrenoceptors%5BAll+Fields%5D+AND+micad%5Bbook%5D))
- Gene information in NCBI (α_1_-adrenoceptors (http://www.ncbi.nlm.nih.gov/gene?term=alpha%20adrenoceptor%20human), α_2_-adrenoceptors (http://www.ncbi.nlm.nih.gov/gene?term=alpha%20adrenoceptor%20human))
- Articles in OMIM (α_1_-adrenoceptors (http://omim.org/search?index=entry&start=1&limit=10&search=alpha-1-adrenergic+receptor&sort=score+desc+%2C+prefix_sort+desc&sort=score+desc+%2C+prefix_sort+desc), α_2_-adrenoceptors (http://omim.org/search?index=entry&start=1&limit=10&search=alpha-2-adrenergic+receptor&sort=score+desc+%2C+prefix_sort+desc&sort=score+desc+%2C+prefix_sort+desc))
- Clinical trials ([^11^C]Mirtazapine (http://www.clinicaltrials.gov/ct2/show/NCT00288782?term=Mirtazapine+PET&rank=1))
- Drug information in FDA (Mirtazapine (http://google2.fda.gov/search?q=Mirtazapine&client=FDAgov&site=FDAgov&lr=&proxystylesheet=FDAgov&output=xml_no_dtd&getfields=*&x=5&y=12))

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=11C%20Mirtazapine%20and%20synthesis)]

[^11^C]Mirtazapine was synthesized remotely via a reaction of [^11^C]methyl iodine with desmethyl precursor in the presence of NaOH (8). [N-Methyl-^11^C]mirtazapine was purified by high-performance liquid chromatography (HPLC) with a radiochemical yield of 21% (end of synthesis). The radiochemical purity was >98%, and the specific activity was 5-7 GBq/μmol (0.14-0.19 Ci/μmol) at end of synthesis. Time of synthesis was 35 min (end of bombardment).

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=11C%20Mirtazapine%20and%20in%20vitro)]

On the basis of in vitro competition binding studies, Marthi et al. (9) reported pK_i_ values for mirtazapine of 7.3 for α_2_-adrenoceptors ([^3^H]rauwolscine), 6.4 for α_1_-adrenoceptors ([^3^H]prazosin), 4.9 for 5-HT_1_ receptors ([^3^H]serotonin), 8.1 for 5-HT_2_ receptors ([^3^H]mianserin), and 9.3 for histamine-1 receptors ([^3^H]mepyramine).

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=11C%20Mirtazapine%20and%20rodentia)]

No publications are currently available.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=11C%20Mirtazapine%20and%20%28dog%20or%20pig%20or%20rabbit%20or%20sheep%29)]

Marthi et al. (8) performed PET studies in the brain of a normal pig and found high accumulation of radioactivity in the frontal cortex (distribution volume (DV) = 13.4), followed by the thalamus (DV = 11.0), basal ganglia (DV = 9.0), cerebellum (DV = 5.2), and olfactory tubercle (DV = 4.1) 20 min after injection of 454 and 480 MBq (12.3 and 13.0 mCi) of [^11^C]mirtazapine. Radioactive levels in the brain peaked within 10 min of injection. Co-injection of mirtazapine decreased the accumulation in the frontal cortex (DV = 4.3), thalamus (DV = 5.7), and basal ganglia (DV = 5.8) but had little effect in the cerebellum (DV = 4.4) and olfactory tubercle (DV = 3.5). The fraction of unchanged [^11^C]mirtazapine in the blood, as determined by HPLC, was 40% at 40 min.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=11C%20Mirtazapine%20and%20%28primate%20not%20human%29)]

No publications are currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=11C%20Mirtazapine%20and%20human)]

Marthi et al. (10) reported on human PET studies in which [^11^C]mirtazapine (175-413 MBq (4.7-11.2 mCi)) was administered to 5 healthy male volunteers. Various kinetic parameters were estimated by nonlinear regression using one-tissue compartment. The DVs of [^11^C]mirtazapine were markedly greater in the hippocampus and amygdala (11.3-12.0), followed by the temporal cortex (10.9), occipital cortex (9.9), striatum (9.7), frontal cortex (9.5), thalamus (9.4), and cerebellum (6.7). The fraction of unchanged [^11^C]mirtazapine in the blood, as determined by HPLC, was 30-60% at 25 min and 20-40% at 60 min.

Marthi et al. (11) reported on PET scans in a healthy, 43-year-old female volunteer (weight, 68 kg) after injection of 326 MBq (8.8 mCi) of [^11^C]mirtazapine. Absorbed doses were found to be 34 μGy/MBq (0.12 rad/mCi) for the lungs, 18.5 μGy/MBq (0.068 rad/mCi) for the liver, 12 μGy/MBq (0.044 rad/mCi) for the adrenals, 12 μGy/MBq (0.044 rad/mCi) for the spleen, 11 μGy/MBq (0.041 rad/mCi) for the gallbladder, 8.2 μGy/MBq (0.03 rad/mCi) for the heart wall, and 8.0 μGy/MBq (0.03 rad/mCi) for the brain. The effective dose was 6.8 μSv/MBq (25.2 mrem/mCi).

## References

1 Heusch G. (1990). Alpha-adrenergic mechanisms in myocardial ischemia. Circulation.
2 Brodde O.E. (1991). Beta 1- and beta 2-adrenoceptors in the human heart: properties, function, and alterations in chronic heart failure. Pharmacol Rev.
3 Bristow M.R., Minobe W., Rasmussen R., Larrabee P., Skerl L., Klein J.W., Anderson F.L., Murray J., Mestroni L., Karwande S.V., et al. (1992). Beta-adrenergic neuroeffector abnormalities in the failing human heart are produced by local rather than systemic mechanisms. J Clin Invest.
4 Pascual J., del Arco C., Gonzalez A.M., Pazos A. (1992). Quantitative light microscopic autoradiographic localization of alpha 2-adrenoceptors in the human brain. Brain Res.
5 Callado L.F., Meana J.J., Grijalba B., Pazos A., Sastre M., Garcia-Sevilla J.A. (1998). Selective increase of alpha2A-adrenoceptor agonist binding sites in brains of depressed suicide victims. J Neurochem.
6 de Boer T. (1996). The pharmacologic profile of mirtazapine. J Clin Psychiatry.
7 Kent J.M. (2000). SNaRIs, NaSSAs, and NaRIs: new agents for the treatment of depression. Lancet.
8 Marthi K., Bender D., Gjedde A., Smith D.F. (2002). [11C]Mirtazapine for PET neuroimaging: radiosynthesis and initial evaluation in the living porcine brain. Eur Neuropsychopharmacol.
9 de Boer T.H., Maura G., Raiteri M., de Vos C.J., Wieringa J., Pinder R.M. (1988). Neurochemical and autonomic pharmacological profiles of the 6-aza-analogue of mianserin, Org 3770 and its enantiomers. Neuropharmacology.
10 Marthi K., Jakobsen S., Bender D., Hansen S.B., Smith S.B., Hermansen F., Rosenberg R., Smith D.F. (2004). [N-methyl-11C]Mirtazapine for positron emission tomography neuroimaging of antidepressant actions in humans. Psychopharmacology (Berl).
11 Marthi K., Hansen S.B., Jakobsen S., Bender D., Smith S.B., Smith D.F. (2003). Biodistribution and radiation dosimetry of [N-methyl-11C]mirtazapine, an antidepressant affecting adrenoceptors. Appl Radiat Isot.